# N-(4-(4-(2-(2-[^18^F]Fluoroethoxy)phenyl)piperazine-1-yl)butyl)-4-(3-thienyl)benzamide

Chemical name: | N-(4-(4-(2-(2-[^18^F]Fluoroethoxy)phenyl)piperazine-1-yl)butyl)-4-(3-thienyl)benzamide
Abbreviated name: | [^18^F]5
Synonym:
Agent category: | Compound
Target: | Dopamine D_3_ receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically . These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-Like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons. Dopamine receptors are G-protein–coupled receptors and exist in high- and low-affinity states with respect to agonist binding (4). The two states are interconvertible. The high-affinity state is coupled to G-proteins, whereas the low-affinity state is not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiological conditions, dopamine is expected to bind predominantly to the high-affinity state, which is ~50% occupied by 10 nM dopamine. The high-affinity state is suggested to be the functional form of the dopamine receptors.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making studies of extrastriatal D_2/3_ receptors difficult (6-8). In binding studies, ^123^I-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding and to be selective for striatal and extrastriatal D_2_ receptors (9). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors in positron emission tomography (PET) in vivo studies (10-13). [^18^F]Fallypride identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguish between the high- and low-affinity states of the D_2_ receptors. (-)-N-Propyl-norapomorphine (NPA) is reported to have K_high_ and K_low_ values of 0.07–0.4 and 20–200 nM, respectively (3, 4, 14, 15). This provides a >50-fold selectivity for the high-affinity over the low-affinity receptors. NPA has good affinity (K_i_, 0.3 nM) for D_2_ receptors but not for other neurotransmitters (16). [^11^C]NPA is being developed as a PET agent for the noninvasive study of the high-affinity state of the D_2/3_ receptors in the brain. Because of high D_3_ receptor expression in the limbic structures of the brain and possible involvement of striatal D_3_ receptors in the pathophysiology of dystonia, there is a need for D_3_-selective probes. (R)-(-)-2-Chloro-N-[1-^11^C-propyl]n-propylnorapomorphine (2-Cl-[^11^C]-(-)-NPA (http://www.ncbi.nlm.nih.gov/books/NBK50682/)) has been evaluated as a D_3_-selective probe because 2-Cl-(-)-NPA showed a higher selectivity for D_3_ than for D_2_ (D_3_versus D_2_, 3.85) than did (-)-NPA (D_3_versus D_2_, 1.75) (17). However, 2-Cl-[^11^C]-(-)-NPA is less likely to be a useful PET agent for D_3_ receptors because of its slow brain uptake and low striatum/cerebellum ratio. Mach et al. (18) have reported the development of N-(4-(4-(2-(2-[^18^F]fluoroethoxy)phenyl)piperazine-1-yl)butyl)-4-(3-thienyl)benzamide ([^18^F]5), a D_3_ partial agonist, for PET imaging of D_3_ receptors. Compound 5 showed ~162-fold selectivity for D_3_ over D_2_.

### Related Resource Links:

- Chapters in MICAD (Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20synthesis)]

[^18^F]5 was readily synthesized with standard ^18^F-fluorination of the mesylate precursor ([^18^F]KF/Kryptofix 2.2.2, 80°C, 10 min) (18). [^18^F]5 was purified with high-performance liquid chromatography. An overall radiochemical yield was 50% with a specific activity of 55.5 GBq/µmol (1.5 Ci/µmol) at the end of synthesis and a radiochemical purity of >95%. Total synthesis time was ~60 min. Log P_7.4_ (lipophilicity) value was measured to be 4.67.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20in%20vitro)]

Compound 5 exhibited K_i_ values of 27.7 ± 5.4, 0.17 ± 0.01, and 246 ± 13 nM for D_2_, D_3_, and D_4_ (18), respectively. Compound 5 showed ~162-fold selectivity for D_3_ over D_2_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20rodentia)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20%28primate%20not%20human%29)]

Mach et al. (18) performed dynamic PET brain scans for 120 min in four male rhesus monkeys after injection of 18.5 MBq (5 mCi) [^18^F]5. Only one monkey showed a high accumulation in the caudate and putamen, which are known to express D_3_ receptors. The lack of accumulation in the other three monkeys may be due to increased endogenous dopamine with conditions of isoflurane anesthesia. Therefore, lorazepam (1 mg/kg) was injected 30 min before [^18^F]5 to reduce synaptic dopamine in the brain. Tissue time-activity curves showed that lorazepam pretreatment enhanced accumulation of radioactivity in the caudate, thalamus, and putamen in all four monkeys with little effect in the cerebellum. Lorazepam showed little effect on the [^18^F]5 blood curve or metabolism. [^18^F]5 remained ~16% intact at 15 min after injection. Blocking studies were performed with injection of 1 mg/kg compound 6 (a derivative of compound 5 with 124-fold D_3_ selectivity versus D_2_) 5 min before tracer injection in lorazepam-treated monkeys. Binding potential (BP_ND_ = DVR-1) analysis was performed with Logan distribution volume ratio (DVR). The BP_ND_ values for caudate, thalamus, and putamen of lorazepam-treated monkeys were 0.23, 0.21, and 0.14, respectively. Compound 6 reduced their BP_ND_ values to ~0.01.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20human)]

No publications are currently available.

## NIH Support

N01MH32004

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 George S.R., Watanabe M., Di Paolo T., Falardeau P., Labrie F., Seeman P. (1985). The functional state of the dopamine receptor in the anterior pituitary is in the high affinity form. Endocrinology.
5 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
6 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
7 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
8 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
9 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
10 Grunder, G., C. Landvogt, I. Vernaleken, H.G. Buchholz, J. Ondracek, T. Siessmeier, S. Hartter, M. Schreckenberger, P. Stoeter, C. Hiemke, F. Rosch, D.F. Wong, and P. Bartenstein, The Striatal and Extrastriatal D2/D3 Receptor-Binding Profile of Clozapine in Patients with Schizophrenia. Neuropsychopharmacology, 2005
11 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
12 Riccardi P., Li R., Ansari M.S., Zald D., Park S., Dawant B., Anderson S., Doop M., Woodward N., Schoenberg E., Schmidt D., Baldwin R., Kessler R. (2006). Amphetamine-induced displacement of [18F] fallypride in striatum and extrastriatal regions in humans. Neuropsychopharmacology.
13 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
14 Gardner B., Strange P.G. (1998). Agonist action at D2(long) dopamine receptors: ligand binding and functional assays. Br J Pharmacol.
15 Lahti R.A., Mutin A., Cochrane E.V., Tepper P.G., Dijkstra D., Wikstrom H., Tamminga C.A. (1996). Affinities and intrinsic activities of dopamine receptor agonists for the hD21 and hD4.4 receptors. Eur J Pharmacol.
16 Neumeyer J.L., Neustadt B.R., Oh K.H., Weinhardt K.K., Boyce C.B., Rosenberg F.J., Teiger D.G. (1973). Aporphines. 8. Total synthesis and pharmacological evaluation of (plus or minus)-apomorphine, (plus or minus)-apocodeine, (plus or minus)-N-n-propylnorapomorphine, and (plus or minus)-N-n-propylnorapocodeine. J Med Chem.
17 Palner M., McCormick P., Gillings N., Begtrup M., Wilson A.A., Knudsen G.M. (2010). Radiosynthesis and ex vivo evaluation of (R)-(-)-2-chloro-N-[1-11C-propyl]n-propylnorapomorphine. Nucl Med Biol.
18 Mach R.H., Tu Z., Xu J., Li S., Jones L.A., Taylor M., Luedtke R.R., Derdeyn C.P., Perlmutter J.S., Mintun M.A. (2011). Endogenous dopamine (DA) competes with the binding of a radiolabeled D receptor partial agonist in vivo: a positron emission tomography study. Synapse.